# 2-((2-Amino-4-chloro-5-[^18^F]fluorophenyl)thio)-N,N-dimethylbenzenmethanamine

Chemical name: | 2-((2-Amino-4-chloro-5-[^18^F]fluorophenyl)thio)-N,N-dimethylbenzenmethanamine
Abbreviated name: | [^18^F]ACF
Synonym:
Agent Category: | Compound
Target: | Serotonin transporter (SERT)
Target Category: | Ligand binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACF%5BAll%20Fields%5D%20AND%20serotonin)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed]

The neurotransmitter serotonin (5-hydroxytryptamine (5-HT)) plays a major role in a variety of brain functions (e.g., appetite, sleep, and mood). Neuropsychiatric disorders such as major depression, schizophrenia, Alzheimer’s disease, and Parkinson’s disease (1-3) involve a dysfunction of the brain’s serotonin system. The serotonergic neurons – present in wide areas of the brain, including the hypothalamus, thalamus, and cerebral cortex – bear a protein called ”serotonin transporter” (SERT) (4).

SERT, located on the cell bodies and terminals of 5-HT neurons, is a specific marker for the number and integrity of presynaptic terminals of serotonin-producing neurons. It regulates neurotransmission by removing released serotonin from the extracellular space back into the presynaptic neuron. Commonly prescribed antidepressants are selective serotonin reuptake inhibitors, and their effect is obtained through interaction with (and inhibition of) SERT (5). For that reason, in vivo imaging of the regional brain distribution of SERT is an important tool for study of the 5-HT system and the treatment of neuropsychiatric disorders.

A variety of in vivo radioligands for positron emission tomography (PET) have been evaluated for imaging SERT. [^11^C]McN5652 was the first successful and widely used agent (6, 7). However, it does have some limitations related to its slow brain kinetics and low to nonspecific binding ratios in humans. [^11^C]McN5652 is adequate for regions with high SERT density, but because of its high nonspecific binding, it often provides insufficient signal-to-noise differentials for imaging brain regions with intermediate to low SERT densities (e.g., limbic and neocortical regions).

Over recent years, new PET radioligands have been synthesized and evaluated as SERT imaging agents and alternatives to [^11^C]McN5652. Among them, the C-11-labeled tracers N,N-dimethyl-2-(2-amino-4-cyanophenylthio)benzylamine ([^11^C]DASB), 2-(2-(dimethylaminomethyl)phenylthio)-5-fluoromethylphenylamine ([^11^C]AFM) (8), 5-bromo-2-[2-(dimethylaminomethylphenylthio)]phenylamine ([^11^C]DAPA), 2-[2-(dimethylaminomethylphenylthio)]-5-iodophenylamine ([^11^C]ADAM), and N,N-dimethyl-2-(2´-amino-4´-hydroxymethylphenylthio)benzylamine ([^11^C]HOMADAM) (9) are based on a diaryl sulfide motif (4). F-18-labeled radioligands have also been synthesized and investigated (10). Compared with C-11 tracers, they offer better opportunities for data collection and full kinetic analysis. 2-((2-Amino-4-chloro-5-[^18^F]fluorophenyl)thio)-N,N-dimethylbenzenmethanamine ([^18^F]ACF) is a radioligand with the fluorine attached directly to the phenyl ring (for increased stability). It has been proposed as a potential PET tracer for imaging SERT.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACF%5BAll%20Fields%5D%20AND%20serotonin%20AND%20synthesis)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D]

ACF and its F-18 radiolabeling precursor can be prepared according to a multistep procedure described by Oya et al. (11). Briefly, 2,5-dichloro-4-nitrophenylamine is coupled with thiobenzamide to give 2-(5-amino-4-chloro-2-nitrophenylthio)-N,N-dimethylbenzamide. The amino group of this compound is then converted to the fluoride 2-(4-chloro-5-fluoro-2-nitrophenylthio)-N,N-dimethylbenzamide by quenching the diazo intermediate with HPF_6_ followed by thermal decomposition. Finally, the nitro and amide groups of 2-(4-chloro-5-fluoro-2-nitrophenylthio)-N,N-dimethylbenzamide are simultaneously reduced to amines with borane-tetrahydrofuran (THF) to produce ACF.

[^18^F]ACF is obtained via [^18^F]fluoride displacement of its precursor 2-chloro-5-(2-dimethylaminocarbonyl-phenylthio)-4-nitrophenyl)trimethylammonium. This radiolabeling procedure involves mixing the precursor with [^18^F]fluoride in dimethyl sulfoxide at 55 °C for 10 min. This produces the intermediate compound 2-(4-chloro-5-[^18^F]fluoro-2-nitrophenylthio)-N,N-dimethylbenzamide, which is then purified (by Sep-Pak) and reduced via a sequential borane and stannous reduction reaction (BH_3_-THF and SnCl_2_) to produce [^18^F]ACF.

The reported radiochemical purity of [^18^F]ACF produced by this method was >99% (as determined by high-performance liquid chromatography) (11). The reported radiochemical yield at the end of the synthesis was 10-15% (decay corrected), and the specific activity of the radiotracer produced was 37 GBq/mmol (1 Ci/mmol) (11). The total synthesis time, as reported by Oya et al. (11), is about 3 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACF%5BAll%20Fields%5D%20AND%20serotonin%20AND%20in%20vitro)]

Oya et al. (11) performed in vitro binding studies of ACF, using LLC-PK1 cells that over-expressed SERT, dopamine transporter (DAT), or norepinephrine transporter (NET), and showed that ACF had high affinity and good selectivity for SERT. The authors reported inhibition coefficients (K_i_s) of 0.05 ± 0.01, 3020 ± 110 and 650 ± 80 nM for SERT, DAT, and NET, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACF%20AND%20serotonin%20AND%20%22rodentia%22%5BMeSH%20Terms%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%22rodentia%22]

Biodistribution studies in rats were performed by Oya et al. (11). The experimental procedure involved injecting 0.2 ml of saline solution containing 1.1 MBq (30 µCi) of [^18^F]ACF per animal (through the femoral vein) and measuring the uptake of the radiotracer at different time points post injection, after sacrifice.

Results showed excellent uptake of [^18^F]ACF into the brain, with accumulation in regions rich in SERT, such as the striatum, hippocampus, and hypothalamus. Uptake in the hypothalamus reached a peak between 60 and 120 min after injection, a much shorter time compared with the radiotracer [^125^I]ADAM, for which a peak uptake is reached at ~4 h.

The total brain uptakes of [^18^F]ACF at 2, 30, 60, 120, and 240 min post injection reported by Oya et al. (11) were 3.27, 1.28, 0.69, 0.21, and 0.06% of injected dose/organ, respectively. The thalamus/cerebellum activity ratio was 2.37 at 240 min post injection, and the hypothalamus/cerebellum activity ratio was 3.55 at 60 min post injection.

When rats were pretreated with (+)McN5652 (2 mg/kg of tissue) at 5 min before injection of [^18^F]ACF, a significant decrease in specific retention was observed in the striatum, hippocampus, and hypothalamus (at 60 min post injection), suggesting possible competition between [^18^F]ACF and (+)McN5652 for SERT binding sites. On the other hand, no significant difference was observed with pretreatment by nisoxetine or methylphenidate (which do not bind to SERT).

Metabolism studies at 60 post injection showed that almost all of the activity (95 ± 0.40%) extracted from the brain originated from [^18^F]ACF and that metabolites in the peripheral tissues were not likely to play a major role on uptake and retention of the radiotracer (i.e., they are not likely to cross the blood-brain barrier).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACF%20AND%20serotonin%20AND%20%28dog%20OR%20pig%20OR%20sheep%29)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%28dog%20OR%20sheep%20OR%20pig%29]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACF%20AND%20serotonin%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACF%20AND%20serotonin%20AND%20human)]

No publication is currently available.

## References

1 Owens MJ Nemeroff CB The serotonin transporter and depression Depress Anxiety 1998 8Suppl 15 12 9809208
2 Palmer AM, Francis PT, Benton JS, Sims NR, Mann DM, Neary D, Snowden JS, Bowen DM. (1987). Presynaptic serotonergic dysfunction in patients with Alzheimer's disease. J Neurochem.
3 Roth BL, Xia Z. (2004). Molecular and cellular mechanisms for the polarized sorting of serotonin receptors: relevance for genesis and treatment of psychosis. Crit Rev Neurobiol.
4 Laakso A, Hietala J. (2000). PET studies of brain monoamine transporters. Curr Pharm Des.
5 White KJ, Walline CC, Barker EL. (2005). Serotonin transporters: implications for antidepressant drug development. Aaps J.
6 Ichimiya T, Suhara T, Sudo Y, Okubo Y, Nakayama K, Nankai M, Inoue M, Yasuno F, Takano A, Maeda J, Shibuya H. (2002). Serotonin transporter binding in patients with mood disorders: a PET study with [11C](+)McN5652. Biol Psychiatry.
7 Suehiro M, Scheffel U, Ravert HT, Dannals RF, Wagner HN. (1993). [11C](+)McN5652 as a radiotracer for imaging serotonin uptake sites with PET. Life Sci.
8 Huang Y, Hwang DR, Bae SA, Sudo Y, Guo N, Zhu Z, Narendran R, Laruelle M. (2004). A new positron emission tomography imaging agent for the serotonin transporter: synthesis, pharmacological characterization, and kinetic analysis of [11C]2-[2-(dimethylaminomethyl)phenylthio]-5-fluoromethylphenylamine ([11C]AFM). Nucl Med Biol.
9 Jarkas N, Votaw JR, Voll RJ, Williams L, Camp VM, Owens MJ, Purselle DC, Bremner JD, Kilts CD, Nemeroff CB, Goodman MM. (2005). Carbon-11 HOMADAM: a novel PET radiotracer for imaging serotonin transporters. Nucl Med Biol.
10 Huang Y, Bae SA, Zhu Z, Guo N, Roth BL, Laruelle M. (2005). Fluorinated diaryl sulfides as serotonin transporter ligands: synthesis, structure-activity relationship study, and in vivo evaluation of fluorine-18-labeled compounds as PET imaging agents. J Med Chem.
11 Oya S, Choi SR, Coenen H, Kung HF. (2002). New PET imaging agent for the serotonin transporter: [(18)F]ACF (2-[(2-amino-4-chloro-5-fluorophenyl)thio]-N,N-dimethyl-benzenmethanamine). J Med Chem.